# (S)-1-((1-(2-[^18^F]Fluoroethyl)-1H-[1,2,3]-triazol-4-yl)methyl)-5-(2-4-difluorophenoxymethyl-pyrrolidine-1-sulfonyl)isatin

Chemical name: | (S)-1-((1-(2-[^18^F]Fluoroethyl)-1H-[1,2,3]-triazol-4-yl)methyl)-5-(2-4-difluorophenoxymethyl-pyrrolidine-1-sulfonyl)isatin
Abbreviated name: | [^18^F]Isatin-15
Synonym:
Agent category: | Compound
Target: | Caspase-3, caspase-7
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20Isatin)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). Apoptosis is gene-regulated (2) and is the result of proteolysis of intracellular components by activation of a series of proteolytic enzymes called caspases and changes of plasma membrane structure by translocase, floppase, and scramblase (3-5). As a result, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. On the other hand, PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane.

Annexin V is a 36-kDa endogenous human protein produced in particular by epithelial cells from many tissues, such as the placenta, umbilical vessels, liver, spleen, kidney, heart, uterus, and skeletal muscle, as well as by erythrocytes, leukocytes, endothelial cells, and platelets (6). Annexin V binds to PS with high affinity (K_d_ = 7 nM) (3, 7, 8). Apoptosis can be induced by chemicals, radiation, cytokines, hormones, and various pathological conditions (5); therefore, the ability to monitor apoptosis in association with disease progression or regression should provide important information for clinical applications. Annexin V has been radiolabeled with ^18^F, ^123^I, ^125^I, and ^99m^Tc for imaging (9-12). However, annexin V is not able to distinguish between apoptosis and necrosis. However, PS is expressed in both cell necrosis and apoptosis whereas caspase 3/7 activation is only expressed in apoptosis. Caspase substrate may be an attractive alternative for imaging cells undergoing apoptosis because caspases are key enzymes that mediate apoptosis (13). Smith et al. (14) reported that isatin sulfonamide analogs exhibited selective inhibition of caspase-3 and caspase-7 (executioner caspases) over caspase-1, -6, and -8 (initiator caspases). (S)-1-((1-(2-[^18^F]Fluoroethyl)-1H-[1,2,3]-triazol-4-yl)methyl)-5-(2-4-difluorophenoxymethyl-pyrrolidine-1-sulfonyl)isatin ([^18^F]Isatin-15), one of the isatin sulfonamide analogs, has been synthesized for imaging caspase-3/7 activation in apoptosis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Isatin%20and%20synthesis)]

Smith et al. (14) report the synthesis of [^18^F]Isatin-15 by copper catalyzed cycloaddition of 2-[^18^F]fluoroethylazide with the alkyne precursor at room temperature for 30 min. Subsequent high-performance liquid chromatography separation gave radiochemical yields of 65 ± 6% (decay-corrected) and a radiochemical purity of >99%. The specific activity was 1.2 GBq/μmol (32 mCi/μmol) at the end of synthesis (EOS) with the total synthesis and formulation time of 180 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20Isatin+and+in+vitro)]

In vitro caspase enzyme assays using Isatin-15 showed inhibition concentration (IC_50_) values of 0.5 nM for caspase-3, 2.2 nM for caspase-7, and >5,000 nM for caspase-1/6/8 (14). Induction of caspase-3 apoptosis with cisplatin in RIF-1 murine fibrosarcoma cells for 1 h increased accumulation of [^18^F]Isatin-15 of 50% over the untreated cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Isatin%20and%20rodentia)]

Smith et al. (14) performed ex vivo biodistribution studies in RIF-1 tumor-bearing mice (n = 3-6 mice per group) and found rapid accumulation in the liver (~7.5% ID/g), kidneys (~5% ID/g), and lung (~2.5% ID/g) at 2-10 min after injection, followed by rapid elimination from all tissues by 60 min. Radioactivity levels were <0.5% ID/g in all tissues including the bone, blood and tumor at 60 min after injection. The amount of intact [^18^F]Isatin-15 in the plasma was 65% at 60 min after injection with one major hydrophilic radiometabolite. Pretreatment of the tumor-bearing mice (n = 8/group) with cisplatin (10 mg/kg) for 24 h to induce apoptosis significantly increased the accumulation of [^18^F]Isatin-15 in the treated tumors by 190% over the control tumors at 60 min after injection. Effects of cisplatin on the radioactivity levels in other tissues were not reported. No blocking or caspase inhibition experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Isatin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Isatin%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Isatin%20and%20human)]

No publications are currently available.

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Steller H. (1995). Mechanisms and genes of cellular suicide. Science.
3 Thiagarajan P., Tait J.F. (1990). Binding of annexin V/placental anticoagulant protein I to platelets. Evidence for phosphatidylserine exposure in the procoagulant response of activated platelets. J Biol Chem.
4 Song Z., Steller H. (1999). Death by design: mechanism and control of apoptosis. Trends Cell Biol.
5 Blankenberg F.G., Tait J., Ohtsuki K., Strauss H.W. (2000). Apoptosis: the importance of nuclear medicine. Nucl Med Commun.
6 Blankenberg F.G., Strauss H.W. (2001). Will imaging of apoptosis play a role in clinical care? A tale of mice and men. Apoptosis.
7 van Heerde W.L., de Groot P.G., Reutelingsperger C.P. (1995). The complexity of the phospholipid binding protein Annexin V. Thromb Haemost.
8 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
11 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
12 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
13 Neuss M., Crow M.T., Chesley A., Lakatta E.G. (2001). Apoptosis in cardiac disease--what is it--how does it occur. Cardiovasc Drugs Ther.
14 Smith G., Glaser M., Perumal M., Nguyen Q.D., Shan B., Arstad E., Aboagye E.O. (2008). Design, synthesis, and biological characterization of a caspase 3/7 selective isatin labeled with 2-[18F]fluoroethylazide. J Med Chem.